# (2S,αS)-2-(α-(2-[^125^I]Iodophenoxy)benzyl)morpholine

Chemical name: | (2S,αS)-2-(α-(2-[^125^I]Iodophenoxy)benzyl)morpholine
Abbreviated name: | (S,S)-[^125^I]IPBM
Synonym: | (2S)-2-[(S)-(2-Iodanylphenoxy)-phenylmethyl]morpholine
Agent category: | Compound
Target: | Norepinephrine transporter (NET)
Target category: | Transporter
Method of detection: | Single-photon emission computed tomography, gamma planar imaging
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM)]

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathological changes of adrenergic transmission has been an important area of radiopharmaceutical research (1, 2). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (3). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (4). All of the NE adrenergic receptors belong to the G-protein–linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals, and it is responsible for active reuptake (uptake-1) of NE released from neurons (5). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (6). Brain NET is involved in various neurological and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (7). NET is also the site of action in the brain for many antidepressant drugs (8).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (4). [^123^I]-meta-Iodobenzylguanidine, [^11^C]meta-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (9). However, this class of tracers is not suitable for the study of the brain NET system because they are not able to cross the blood–brain barrier (10). In the brain, NET levels are relatively low compared with those of other transporters, such as dopamine transporter (DAT) and serotonin transporter (SERT) (8). Several NET reuptake inhibitors such as [^11^C]desipramine have been tested, but they showed high nonspecific binding. Reboxetine ((RS)-2-[((RS)-2-ethoxyphenoxy)benzyl]morpholine) is a specific NET inhibitor with a high affinity and selectivity. Reboxetine is available as a racemic mixture of the (R,R) and (S,S) enantiomers. The (S,S) enantiomer has been found to be more potent, with a 50% inhibition concentration (IC_50_) value of 3.6 nM, for inhibiting NET in rat hypothalamic synaptosomes. Among the different reboxetine derivatives that have been tested, (2S,αS)-2-(α-(2-[^125^I]iodophenoxy)benzyl)morpholine ((S,S)-[^125^I]IPBM) is considered a potential candidate to be developed as a single-photon emission computed tomography (SPECT) ligand for studying the brain and heart NET system (11, 12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20synthesis)]

Kanegawa et al. (11) reported the radiosynthesis of (S,S)-[^125^I]IPBM by a halogen exchange reaction with ^125^I (2S, 3S). -2-[α-(2-bromophenoxy)benzyl]morpholine was reacted with [^125^I]NaI in the presence of ammonium sulfate and copper(II) sulfate pentahydrate. The mixture was heated for 45 min at 130ºC. Radiochemical yields were 65%. After purification with high-performance liquid chromatography, the final product had a radiochemical purity of >98%. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20in%20vitro)]

Kanegawa et al. (11) showed that inhibition constant (K_i_) values of nisoxetine (NET inhibitor), fluoretine (SERT inhibitor), and GBR12909 (DAT inhibitor) were 4.17 ± 1.98, 1,073 ± 437, and >5,000 nM, respectively. The binding assays were performed using the cerebral cortex of male rats and (S,S)-[^125^I]IPBM. The selectivity ratio of SERT to NET (K_i_ SERT/K_i_ NET) was 257 and of DAT to NET (K_i_ DAT/K_i_ NET) was >1,000. (S,S)-[^125^I]IPBM had a binding affinity (K_d_) of 1.30 ± 0.46 nM.

Kiyono et al. (12) showed that 50% inhibition concentration (IC_50_) values of nisoxetine, fluoretine, and GBR12909 were 2.28 ± 0.87, 1,165 ± 204, and >10,000 nM, respectively. The binding assays were performed using rat heart membranes and (S,S)-[^125^I]IPBM. The selectivity ratio of SERT to NET was 511 and of DAT to NET was >4,000. (S,S)-[^125^I]IPBM had a K_d_ value of 1.62 ± 0.22 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20rodentia)]

Kanegawa et al. (11) performed ex vivo biodistribution studies in normal rats (n = 4/group) after injection of (S,S)-[^125^I]IPBM. (S,S)-[^125^I]IPBM rapidly entered the brain, and the levels of radioactivity in the brain, measured as percent injected dose per gram (% ID/g), was 0.44, 0.51, 0.54, 0.43, and 0.25 at 5, 15, 30, 60, and 180 min after injection, respectively. The radioactivity in blood cleared rapidly. The brain/blood ratio was 14.3 at 60 min after the injection. The organ with the highest initial uptake (5 min after injection) was the lung (5.0% ID/g), followed by the adrenal gland (1.4% ID/g) and kidneys (1.0% ID/g) with gradual to moderate washout rate. The radioactivity that accumulated in the intestines and stomach showed prominent increases at 30–60 min after injection, whereas the radioactivity in the liver was low (<0.3% ID/g). Furthermore, there was low accumulation in the thyroid gland with 0.01% ID/g at 5 min and 0.04% ID/g at 180 min after injection. The radioactivity level in the heart was not measured. Regional brain biodistribution showed a high accumulation in the thalamus, midbrain, cerebellum, and pons (NET-rich regions) and a low accumulation in the striatum. The accumulation of radioactivity in the NET-rich regions peaked at ~30 min after injection. The ratio of radioactivity in the NET-rich regions to the striatum was greatest at 180 min. Ex vivo autoradiographic analyses showed that the highest levels of radioactivity were observed in the locus coeruleus and anteroventricular thalamic nucleus. Co-administration of 10 mg/kg nisoxetine with (S,S)-[^125^I]IPBM reduced radioactivity levels in the NET-rich regions by >80% in all organs except the striatum. Fluoxetine (10 mg/kg) and GBR12909 (1 mg/kg) exhibited no reduction of radioactivity levels in the NET-rich regions.

Kiyono et al. (12) reported that there was a rapid and moderate uptake of (S,S)-[^125^I]IPBM by the heart (0.64% ID/g at 60 min) in rats. The heart/blood ratio increased with time, with a maximum value of 31.9 at 180 min after injection. Co-administration of nisoxetine (1 mg/kg) with (S,S)-[^125^I]IPBM led to a 60% reduction in radioactivity level in the heart, whereas fluoxetine (1 mg/kg) and GBR12909 (1 mg/kg) exhibited little effect.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20%28primate%20NOT%20human%29)]

Kanegawa et al. (11) evaluated (S,S)-[^125^I]IPBM as a radioligand for SPECT imaging studies of brain NET in a female common marmoset with 222 MBq (6 mCi) (S,S)-[^125^I]IPBM. Imaging studies showed high accumulation in the thalamus, cortex, and cerebellum (NET-rich regions) and low accumulation in the striatum. Treatment with nisoxetine (5 mg/kg) at 68 min after (S,S)-[^125^I]IPBM injection led to reduced radioactivity levels in the NET-rich regions but not in the striatum. The radioactivity levels in the NET-rich regions were reduced to that of the striatum at 211 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IPBM%20AND%20human)]

No publication is currently available.

## References

1 Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
2 Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
3 Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
4 Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
5 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
6 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
7 Zahniser N.R., Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
8 Wilson A.A., Johnson D.P., Mozley D., Hussey D., Ginovart N., Nobrega J., Garcia A., Meyer J., Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
9 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
10 Ding Y.S., Lin K.S., Logan J., Benveniste H., Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
11 Kanegawa N., Kiyono Y., Kimura H., Sugita T., Kajiyama S., Kawashima H., Ueda M., Kuge Y., Saji H. (2006). Synthesis and evaluation of radioiodinated (S,S)-2-(alpha-(2-iodophenoxy)benzyl)morpholine for imaging brain norepinephrine transporter. Eur J Nucl Med Mol Imaging.
12 Kiyono Y., Sugita T., Ueda M., Kawashima H., Kanegawa N., Kuge Y., Fujibayashi Y., Saji H. (2008). Evaluation of radioiodinated (2S,alphaS)-2-(alpha-(2-iodophenoxy)benzyl)morpholine as a radioligand for imaging of norepinephrine transporter in the heart. Nucl Med Biol.